# Gadolinium-incorporated mesoporous silica nanoparticles

Chemical name: | Gadolinium-incorporated mesoporous silica nanoparticles
Abbreviated name: | Gd_2_O_3_@SiO_2_
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Gadolinium (Gd)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=silica%20nanoparticles%20and%20contrast%20agents)]

The gadolinium (Gd^3+^)-incorporated mesoporous silica nanoparticle (NP), abbreviated as Gd_2_O_3_@SiO_2_, is a non-targeted contrast agent developed by Shao et al. for magnetic resonance imaging (MRI) of tumors (1).

The application of NPs in molecular imaging and drug delivery is currently undergoing a tremendous expansion because of the unique features of NPs, including high stability, high carrier capacity, incorporation feasibility of both hydrophilic and hydrophobic substances, controlled release of drug payloads, and biocompatibility (2-5). The design of NP-based paramagnetic contrast agents must meet certain criteria, which are different from the criteria for the development and use of NPs in drug delivery. For example, paramagnetic metals incorporated into the NPs should be easily accessed by a large number of labile water molecules (6, 7). NP agents must also be stable and safe when used in clinic, and must exhibit isotropic and slow tumbling motion when used in vivo. Silica inorganic NPs are well qualified for use in contrast agent development because they have a mesoporous structure, their sizes can be tuned from 1.5 nm to 30 nm, and they offer large surface areas (>1,000 m^2^/g) for ligand conjugation (5, 6).

Functionalization of the internal surface of silica NPs via the use of alkoxysilanes allows the surface properties to be tailored for various purposes. In general, Gd^3+^-labeled silica NPs are designed either by incorporating Gd^3+^ into silica or by grafting Gd^3+^-chelates onto the NP surface (6, 7). Incorporating Gd^3+^ into silica results in contrast agents with a high relaxivity because of the high payload of Gd^3+^ and the slow tumbling motion of the NPs. Grafting Gd^3+^-chelates onto the NP surface may limit the Gd^3+^ loading because of the reduced number of available anchoring sites on the NP surface. MRI studies have confirmed the usefulness of silica NP-based contrast agents in animal models of human disease. However, numerous questions remain to be addressed for their application in humans. Because the synthetic methods and the nanomaterials for synthesis are highly versatile, it is difficult to determine the relationship between the chemical physical properties of NPs and their in vivo behaviors. The ultimate fate and toxicity of NPs themselves and their metabolites are still poorly understood (7, 8).

As discussed in detail by Fadeel and Garcia-Bennett, silica NPs are commonly prepared by the sol-gel process, which generates silica NPs through the hydrolysis and polycondensation of silicon alkoxide (7). The sol-gel technique is also popular for the synthesis of other types of NPs because the NP properties, such as particle size, pore size, amount of incorporated metals, and surface functional groups, can be easily controlled (4, 7). Synthesis of NPs with the sol-gel technique is also cost-effective on the laboratory scale. Shao et al. reported a one-step synthesis of Gd^3+^-incorporated silica NPs (Gd_2_O_3_@SiO_2_) with a mesoporous structure and high surface area (1). The NPs possess desirable MRI contrast enhancement properties, making them suitable for potential application as target-specific contrast agents for molecular MRI. This chapter summarizes data regarding Gd_2_O_3_@SiO_2_ (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21504064)]

Shao et al. described the one-step synthetic process for producing Gd_2_O_3_@SiO_2_ NPs, which was optimized with a systematic orthogonal test approach (1). Briefly, surfactant pluronic P-123 was first dissolved in distilled water. Reagents HCl, tetraethoxysilane, GdCl_3_·6H_2_O, and an ammonium hydroxide solution were then added sequentially and allowed to react for several minutes to several hours after addition of each reagent. The generated Gd_2_O_3_@SiO_2_ NPs were centrifuged, washed, and dried in air for 12 h at 60°C, and the NPs were then calcined for 6 h at 500°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21504064)]

Shao et al. characterized Gd_2_O_3_@SiO_2_ NPs with different techniques (1). Under transmission electron microscopy, Gd_2_O_3_@SiO_2_ NPs presented an intragranular network morphology. The mean diameter of the NPs was 29.18 nm. Dark and bright spots could be observed in the network with energy dispersive x-ray spectroscopy. The dark spots were determined to be Gd-rich areas with an atomic fraction of 3.42% Gd, and the bright spots were Gd-depleted areas primarily composed of SiO_2_. The overall Gd concentration was measured with inductively coupled plasma-atomic emission spectrometry to be 1.547 (atom.%). N_2_ adsorption–desorption isotherms of NPs before and after incorporation of Gd^3+^ exhibited a typical type IV curve with a clear hysteresis loop. The starting relative pressure for the loop shifted from 0.5 to 0.7, the pore size increased from 7.0 nm to 12.6 nm, and the surface area decreased from 644.9 m^2^/g to 236.9 m^2^/g with the introduction of Gd^3+^. The increase in pore size and the decrease in surface area may be caused by the partial destruction of the mesoporous structure when Gd_2_O_3_ clusters precipitate in the mesoporous silica. No free Gd ions were detected after the Gd_2_O_3_@SiO_2_ NPs were dissolved in phosphate-buffered saline at a concentration of 157.25 mg Gd/L and stored for 48 h at 37.5°C. These results indicate that Gd^3+^ is incorporated into the silica framework, that the structure of the Gd_2_O_3_@SiO_2_ NPs is mesoporous, and that the NPs are stable in vitro (1).

In vitro T1-weighted phantom images at 1.5 T showed that Gd_2_O_3_@SiO_2_ NPs generated a higher signal intensity and had a larger T1 relaxivity than commercial Gd-labeled diethylene triaminepentaacetic acid (Gd-DTPA) (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21504064)]

MRI with Gd_2_O_3_@SiO_2_ NPs was performed in mice bearing subcutaneous xenografts of CNE-2 tumor cells (nasopharyngeal carcinoma cells) (1). T1-Weighted images were obtained at different times after administration of 100 µl of 100 mg/ml NPs or saline via the tail vein. Significant signal enhancement was observed in the livers from mice treated with Gd_2_O_3_@SiO_2_ NPs from 15 min after injection, and the enhancement lasted for >24 h. The tumor xenografts exhibited increased signal intensity starting at 30 min after injection. Detailed data for the in vivo studies, especially for the dynamic enhancement of tumors, were not provided.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Shao Y.Z., Liu L.Z., Song S.Q., Cao R.H., Liu H., Cui C.Y., Li X., Bie M.J., Li L. (2011). A novel one-step synthesis of Gd3+-incorporated mesoporous SiO2 nanoparticles for use as an efficient MRI contrast agent. Contrast Media Mol Imaging.
2 Huang, H.C., S. Barua, G. Sharma, S.K. Dey, and K. Rege, Inorganic nanoparticles for cancer imaging and therapy. J Control Release, 2011
3 Parveen, S., R. Misra, and S.K. Sahoo, Nanoparticles: a boon to drug delivery, therapeutics, diagnostics and imaging. Nanomedicine, 2011
4 Zhao Y., Vivero-Escoto J.L., Slowing, Trewyn B.G., Lin V.S. (2010). Capped mesoporous silica nanoparticles as stimuli-responsive controlled release systems for intracellular drug/gene delivery. Expert Opin Drug Deliv.
5 Rosenholm J.M., Sahlgren C., Linden M. (2011). Multifunctional mesoporous silica nanoparticles for combined therapeutic, diagnostic and targeted action in cancer treatment. Curr Drug Targets.
6 Terreno E., Castelli D.D., Viale A., Aime S. (2010). Challenges for molecular magnetic resonance imaging. Chem Rev.
7 Fadeel B., Garcia-Bennett A.E. (2010). Better safe than sorry: Understanding the toxicological properties of inorganic nanoparticles manufactured for biomedical applications. Adv Drug Deliv Rev.
8 Napierska D., Thomassen L.C., Lison D., Martens J.A., Hoet P.H. (2010). The nanosilica hazard: another variable entity. Part Fibre Toxicol.